# Trisodium-[(2-(R)-[(4,4-diphenylcyclohexyl)phosphono-oxymethyl]-diethylenetriaminepentaacetato)(aquo)gadolinium(III) Gadofosveset

Chemical name: | Trisodium-[(2-(R)-[(4,4-diphenylcyclohexyl)phosphono-oxymethyl]-diethylenetriaminepentaacetato)(aquo)gadolinium(III)
Abbreviated name: | Gadofosveset
Synonym: | MS-325, MS-32520, Vasovist®, AngioMARK, ZK236018
Agent category: | Compound
Target: | Albumin
Target category: | Acceptor
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadofosveset)]

The conventional x-ray angiography (XRA) provides a gold standard for diagnosis of vascular diseases (1). However, this technique requires administration of a large volume of iodinated contrast media through arterial puncture and exposes patients to a significant dose of ionizing radiation. Magnetic resonance imaging (MRI) is a non-invasive alternative to XRA that derives signals from tissue water protons without irradiation (1, 2). The difference between the signal intensity of vasculatures and that of surrounding tissues creates contrasts in MR images and results in a MR angiogram. The use of blood pool contrast agents (BPCAs) enhances the signal in vasculatures and improves the quality of MR angiograms (3). BPCAs are paramagnetic contrast agents designed to remain in the blood for a prolonged time compared to conventional contrast agents like gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA) (3). BPCAs normally include macromolecules attached gadolinium chelates or iron oxide nanoparticles that are sufficiently large to prevent them from diffusing through the endothelium of normal tissue and entering the interstitial space easily. These agents can produce persistent signal-enhancing effects in a much longer acquisition time window to yield better signal-to-noise ratio and image spatial resolution. The difference between their molecular size and the pore size in the capillary endothelium of organs determines their biodistribution and elimination (3). Glomerular capillaries in the kidneys are fenestrated with pores 60–70 nm in diameter, allowing for rapid excretion of molecules <20 kDa regardless of their charges. Molecules between 20 and 70 kDa are partly or completely excreted through the kidney endothelial membrane depending on pH, lipid solubility, and polarity. Molecules >70 kDa do not pass through the glomerulus filter but are metabolized before excretion. For instance, albumin-(DTPA)_30_ has a plasma elimination time of 3.63 h in rats and takes ~1 month to excrete most of the gadolinium after biodegradation (3). In clinical applications, tissue retention–induced toxicity becomes a primary critical factor for the use of BPCAs.

Trisodium-[(2-(R)-[(4,4-diphenylcyclohexyl)phosphono-oxymethyl] diethylenetriaminepenta-acetato)(aquo)gadolinium(III) (Gadofosveset) is a small chelate made from substituted Gd-DTPA. By binding to serum albumin in blood plasma, gadofosvesets are converted to BPCAs as macromolecules attached gadolinium chelates (4). As a well-documented 66-kDa globular protein, human serum albumin (HSA) has several specific binding sites (5). Because this protein is distributed 4.5% in blood plasma, which weighs four times more than interstitial fluid (6), HSA becomes a primary binding target for small paramagnetic chelates to generate BPCAs in situ. The specific binding site II on HSA is located in a hydrophobic cavity of 8–10 Å in diameter and has been a preferential binding site for many ligands, such as fenbufen, diazepam, and piroxicam, in drug designs (5). Gadofosveset comprises a diphenylcyclohexyl moiety attached by a phosphodiester link to Gd-DTPA to fit the specific binding site II (7). The addition of the phosphodiester group increases the hydrophilicity of the complex and the binding affinity (7). This lipophilic diphenylcyclohexyl group also enhances the thermodynamic stability and the kinetic inertness of gadofosveset compared to that of Gd-DTPA, the parent analog (8). The interaction between HSA and gadofosveset is a reversible non-covalent binding, and the equilibrium between the free and the protein-bound fraction always leaves a small amount of free fraction present (9). Such kinetics reduces the leakage of gadofosveset out of the intravascular space, but there still remains an excretion path for the free fraction filtered through the kidneys or via uptake by hepatocytes (9). The non-covalent linking overcomes the tissue retention problem found in other synthetic BPCAs like albumin-(DTPA)_30_. On the other hand, the bound fraction is hidden from the kidneys and leads to an extended plasma half-life. By binding to HSA via multiple groups, the T_1_ relaxivity of gadofosveset increases 4–10 times because of an elongation of rotation correlation time (τ_R_) (9). This enhancement effect is substantially greater than the two- to four-fold increase in efficacy normally found in those gadolinium chelates that are covalently linked to macromolecules (3). Potential applications in clinics include enhancement of vessels in MR angiography and determination of tissue perfusion, angiogenesis, or capillary integrity (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadofosveset+AND+synthesis)]

Farooki et al. described a detailed synthesis of gadofosveset (7). 4,4-Diphenylcyclohexane-1-ol was reacted with 1-(R)-hydroxymethyl-DTPA-penta-tert-butyl ester in 1H-tetrazole at room temperature and yielded a phosphoramidite. This precursor was converted to the corresponding phosphate derivative ((R)-phosphono-oxymethyl-penta-tert-butyl-DTPA) by adding tert-butyl-hydroperoxide in 2 M ammonia in methanol. The resulting compound was treated with Gd_2_O_3_ and sodium hydroxide to produce the trisodium salt of gadofosveset. The molecular weight is 957 Da. Gadofosveset is commercially available (EPIX Medical Inc, MA) and is currently in phase III clinical trials for diagnosis of vascular diseases (1, 2, 10-12).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadofosveset+AND+%22in+vitro%22)]

The relaxation properties of free gadofosveset and albumin-bound gadofosveset were examined with ^1^H nuclear magnetic resonance dispersion spectroscopy (NMRD) at different magnetic field strengths and with ^17^O nuclear magnetic resonance spectroscopy at different temperatures (13). The electron spin relaxation rates of Gd(III) were examined by electron spin resonance spectroscopy (ESR) at X-, Q-, and W-bands (14). Three types of kinetic parameters that determine the proton relaxation rate constants were calculated from these measurements. For the free gadofosveset, the structural water residual time (τ_m_) and the electronic relaxation time (τ_v_) were calculated to be 72 ns and 1.7 ± 0.1 ns, respectively (13). The rotation correlation time (τ_R_) was found to be 115 ps, similar to that of Gd-DTPA. The T_1_ relaxivity for the free gadofosveset was determined to be 7.7 mmol^-1^s^-1^ at 0.47 T at 25°C (13). For the albumin-bound gadofosveset, all three kinetic parameters increased and the values appeared to be sensitive to the structure of albumins, although a considerable sequence homology existed among the albumin proteins from different species (13, 15). With HSA, τ_R_, the structural water exchange rate constant k_ex_ (k_ex_ = 1/τ_m_), and τ_v_ were 8 ± 1 ns, (31 ± 5) × 10^6^ s^-1^, and 6.7 ± 0.3 ns, respectively. With rabbit serum albumin (RSA), τ_R_ and k_ex_ were 13 ± 2 ns and (3.8 ± 0.2) × 10^6^ s^-1^, respectively. These differences were also reflected on the T_1_ relaxivity values measured at 0.47 T and 35°C, which were 46.3 mM^-1^s^-1^ for HSA-bound gadofosveset and 30.5 mM^-1^s^-1^ for RSA-bound gadofosveset. In all cases, the structural hydration number q was found to equal 1 (15).

The binding percentage to albumin varied as a function of gadofosveset concentration. As many as 20 ± 5 gadofosveset molecules were bound to a single HSA molecule at high concentrations, and the strongest site had an association constant on the order of 10^4^ mol^-1^L (16). However, only one or two molecules of gadofosveset on average would be bound per HSA molecule in the clinically relevant concentration range of 0.1–1.0 mM, corresponding to doses of 0.01–0.1 mmol/kg (16). The binding affinity ranged from 67% to 96% and appeared to be varied in different species, as shown in the measurement for 0.1 M gadofosveset in blood plasma or in 4.5% albumin solutions (6, 9).

Preclinical safety was assessed by studying the in vitro genotoxic and mutagenic potential on the levels of gene, chromosome, and genome mutation (17). A series of mutagenicity tests were performed, including the mutagenic activity test in prokaryotic cells systems, the chromosome aberration test in hamster ovary cells, and the mouse micronucleus test (17). The results of these studies did not reveal any evidence of mutagenic potential for gadofosveset.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadofosveset+AND++rodentia)]

Parmelee et al. performed a pharmacokinetic study in rats with three doses of 0.025, 0.05, 0.10 mmol/kg (18). The concentration in blood plasma was measured by gamma counting ^153^Gd-labeled gadofosveset (350–460 μCi/mmol) on whole blood samples. The distribution volume (V_d_) was determined to be 0.254 L/kg for the dose of 0.025 mmol/kg and 0.236 L/kg for the dose of 0.10 mmol/kg. The half-life for the arterial phase was 0.865 min for the dose of 0.025 mmol/kg and 0.917 min for the dose of 0.10 mmol/kg. The equilibrium phase half-life was 22.6 min for the dose of 0.025 mmol/kg and 23.18 min for the dose of 0.10 mmol/kg.

The protein binding kinetics in rats was measured at the 0.10-mmol/kg dose (18). After injection of ^153^Gd-labeled gadofosveset, blood was sampled by cardiac puncture at 5, 20, and 60 min with corresponding protein binding percentages of 77.5%, 84%, and 90.5%, respectively. The biodistribution and elimination in rats were also conducted at this dose with ^153^Gd-labeled gadofosveset (210–220 μCi/mmol) (18). Rats were housed in metallic cages for daily collection of urine and feces and then euthanized at 1 or 7 days after injection. Excised tissue samples (blood, small intestine, muscle, spleen, liver, kidneys, heart, fat, lungs, stomach, brain, femur, and lymph node), urine, and feces were analyzed for ^153^Gd gamma counting. Gadofosveset was efficiently eliminated from rats in urine as free chelates. No significant retention was observed in any organs, and no significant dissociation of the chelate was found in vivo.

Steger-Hartmann et al. conducted a single-dose toxicity study in mice and rats. The lowest lethal dose was found to be 6.0 mmol/kg in mice and 3.0 mmol/kg in rats (17). Systemic tolerance studies with daily repeated intravenous administration were conducted in rats for 4 weeks (17). The lowest dose that led to renal tubular vacuolation in rats was found to be 0.03 mmol/kg. No impairment of kidney function was observed in animals with vacuolated kidney cells. Repeated administration also led to the vacuolation of the macrophages in different tissues of rats at 0.21 mmol/kg. A slight decrease in red blood cell parameters (hemoglobin, hematocrit, erythrocyte count) occurred in rats at 0.01 mmol/kg. Productive and developmental toxicity studies were performed in rats. The effects of gadofosveset were assessed in all phases of reproduction (17), including fertility, early and late embryonic and fetal development, as well as perinatal and postnatal development of the offspring such as F2 generations. No treatment-related adverse effects were noted on reproduction parameters.

Turetschek et al. compared the efficacy of gadofosveset with the synthetic albumin-(Gd-DTPA)_30_ in the assessment of microvascularity in tumors (19). Because of the existence of two molecular forms, the pharmacokinetics of gadofosveset behaved quite differently than that of synthetic albumin-(Gd-DTPA)_30_ and failed to distinguish tumors of different grades. Herborn et al. investigated the enhancement effects of gadofosveset in kidneys and vessel walls in a systemic lupus erythematosus (SLE) mouse model to assess the degree of SLE-induced inflammatory lesions of renal impairment (20). This study used gadofosveset to target albumin-rich inflammatory infiltrations within parenchymal organs like kidneys and demonstrated the potential of using gadofosveset as a MRI marker for the inflammatory damage to parenchymal organs and vessels.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

The pharmacokinetic study in rabbits was performed at two doses of 0.025 and 0.10 mmol/kg (18). The concentration in blood plasma was measured by gamma counting ^153^Gd-labeled gadofosveset (210–1,000 μCi/mmol) on whole blood samples. The V_d_ was determined to be 0.114 L/kg for the dose of 0.025 mmol/kg and 0.137 L/kg for the dose of 0.10 mmol/kg. The half-life for the arterial phase was 3.35 min for the dose of 0.025 mmol/kg and 2.84 min for the dose of 0.10 mmol/kg. The equilibrium phase half-life was 174.6 min for the dose of 0.025 mmol/kg and 118 min for the dose of 0.10 mmol/kg. The protein binding kinetics in rabbits was measured at the 0.10-mmol/kg dose (18). After injection of ^153^Gd-labeled gadofosveset, blood samples were collected at 5, 30, and 60 min, and the corresponding protein binding percentage was found in the range of 90% to 96%. Reproductive and development toxicity studies were conducted in rabbits, and the effects of gadofosveset were assessed in all phases of reproduction. Weak sign of maternal toxicity was observed at doses of 0.8 and 2.0 mmol/kg (17). Embryotoxicity and local tolerance studies were also conducted in rabbits (17).

The rabbit blood T_1_ at 1.0 T was reduced to 50–100 ms for 1 h after injection of 0.1 mmol/kg gadofosveset compared to the 400–800 ms for Gd-DTPA (6). The enhancement of the vessel signal appeared to be dose-dependent. Doses as low as 0.015 mmol/kg already exhibited a greatly improved enhancement in contrast, but the signal enhancement reached a plateau at 0.05 mmol/kg. At the 0.025-mmol/kg dose, the vessel signal intensity increased ~400% for at least 1 h after injection. Both small and large vessels exhibited strong enhancement effects. However, the 0.1-mmol/kg dose did not provide a dramatic increase in signal intensity over the dose of 0.05 mmol/kg. In comparison, Gd-DTPA at four times that dose showed poor small-vessel enhancement and short-term enhancement in large-vessels, and only a maximum of 200% increase appeared at ~5 min. Gadofosveset was used to examine stenosed or occluded vessels in pigs at doses of 0.1–0.3 mmol/kg (21) and the first-pass renal perfusion in pigs at a dose of 0.05 mmol/kg (22). Both studies presented a significant improvement to the vascular signals. Herborn et al. demonstrated the capability of improving interstitial MR lymphography with gadofosveset in rabbit tumor models (23).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadofosveset+AND+(primate+non+human))]

Parmelee et al. performed a pharmacokinetic study in monkeys at two doses of 0.025 and 0.10 mmol/kg (18). The concentration in blood plasma was measured by gamma counting ^153^Gd-labeled Gadofosveset (210–1,000 μCi/mmol) on whole blood samples. The V_d_ was determined to be 0.13 L/kg for the dose of 0.025 mmol/kg and 0.144 L/kg for the dose of 0.10 mmol/kg. The half-life for the arterial phase was 4.66 min for the dose of 0.025 mmol/kg and 2.66 min for the dose of 0.10 mmol/kg. The equilibrium phase half-life was 211.6 min for the dose of 0.025 mmol/kg and 142.6 min for the dose of 0.10 mmol/kg. The protein binding kinetics in anesthetized monkeys was measured at the 0.10-mmol/kg dose by quantitative gamma camera scintigraphy. After injection of ^153^Gd-labeled gadofosveset, blood was collected at multiple time points, and the corresponding protein binding percentage was found to be in the range of 80% to 85%. The monkey blood T_1_ at 1.0 T was reduced to 50–100 ms for 1 h after injection of 0.1 mmol/kg (6). In comparison, the T_1_ for Gd-DTPA was 200–500 ms. The pharmacokinetic study was also conducted in baboons and gave similar results (18).

Biodistribution in monkeys was determined by gamma counting ^153^Gd for at least 2 h after injection of 0.1 mmol/kg gadofosveset (18). The percentage of injection dose (ID) in heart, liver, kidneys, and bladder was determined by region-of-interest analysis of scintigraphic images. Excretion in monkeys via urine and feces was determined for 0 to 24, 24 to 48, and 48 to 72 h after injection. On the basis of visualization of both kidneys and strong bladder activity by 5 min after injection, primary elimination in monkeys was found to be through the renal system. For the doses of 0.025 and 0.10 mmol/kg, 78% ID and 90% ID excreted during the first 24 hr, respectively; 84% ID and 92% ID excreted in 72 hr, respectively. Gadofosveset had minimal hepatobiliary excretion in these higher mammals. The long plasma half-life of gadofosveset in monkeys was attributable not only to the low free concentration available for renal excretion but also the lack of hepatocellular uptake.

In acute administration studies in monkeys, mortality was not observed in doses ≤3.0 mmol/kg (17). Clinical observations included excess salivation at 1.0 mmol/kg and retching at 3.0 mmol/kg. No toxicologically significant effects appeared on clinic chemistry, urinalysis parameters, body, or organ weights. Small foci of vacuolation in lymph nodes were found after 140 days at doses ≥1.0 mmol/kg, and the kidney remained in the normal range during this period. Systemic tolerance studies were conducted in monkeys with daily repeated intravenous administration over 4 weeks. Gadofosveset was well tolerated in the monkeys and no deaths were reported. No vacuolation of the macrophages in different tissues was observed with doses up to 0.1 mmol/kg. Red blood cell parameters appeared to decrease slightly at 0.5 mmol/kg, including hemoglobin, hematocrit, and erythrocyte count.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadofosveset+AND+human)]

Phase I clinical trials were conducted in 63 normal subjects to investigate the escalation of doses ranging from 0.05 to 0.15 mmol/kg (16). All participants demonstrated an adequately safe profile with no serious adverse reactions. Mild adverse events were observed, such as nausea and paresthesia. Grist et al. reported the details of a phase I clinical trial in seven health volunteers for imaging peripheral and carotid vessels (24). Steady-state and dynamic MR angiography were performed on a 1.5-T imager at a dose of 0.05 mmol/kg. Standard clinical evaluations (serum chemistry, hematology, urinalysis, iron binding, and clotting) were performed at 0, 3, 12, 24, 36, and 144 hr after administration of gadofosveset. No clinically relevant changes occurred in laboratory evaluations. The dynamic MR angiograms exhibited clear enhancement of major arterial structures, including the femoral artery, deep femoral artery, and three branches of the lateral circumflex femoral artery. The steady-state MR angiograms allowed differentiation of vessel walls from arterial and venous lumina, and clear visualization of branch points, curving vessels, and small vessels.

Phase II clinical trials were conducted in 240 patients at 20 centers in North America to examine the safety and efficacy in diagnosis of peripheral vascular disease (25). The effectiveness of gadofosveset-enhanced MR angiography was compared with that of conventional MR angiography or XRA at five doses of 0.005, 0.01, 0.03, 0.05, and 0.07 mmol/kg. The diagnostic accuracy for detection of aortoiliac occlusive disease increased as the dose increased and reached to a plateau at a dose of 0.03 mmol/kg. At doses ≥0.03 mmol/kg, the gadofosveset-enhanced MR angiography showed a 20% increase in accuracy over the non-enhanced MR angiography for diagnosis of clinically significant aortoiliac occlusive disease compared to XRA. Gadofosveset exhibited a good safety profile in all dose groups with the exception of three serious adverse events possibly related to the drugs, including one case of urticaria, one case of chest pain, and one sudden death. No significant change was observed in blood serum chemistry values. In another multicenter, phase II trial, safety and efficacy of gadofosveset were examined in 26 patients at three doses of 0.01, 0.03, and 0.05 mmol/kg (26). Safety, including clinical laboratory changes and electrocardiographic monitoring, was assessed until 3 d after injection. No deaths or serious adverse events occurred. Two patients receiving the 0.05-mmol/kg dose experienced five mild adverse events within 3 h of injection, including nausea, cramps, metallic taste, and pruritus. On the 5-min images, sensitivity, specificity, and accuracy were 100%, 100%, and 100%; 63%, 100%, and 88%; and 40%, 75%, and 55% at 0.01, 0.03, and 0.05 mmol/kg, respectively.

Phase III clinical trails were performed to examine the diagnostic accuracy and effectiveness for vascular disease at the 0.03-mmol/kg dose compared to conventional MR angiography and XRA (27). A total of 672 patients from 50 sites in the United States, Canada, and Europe were included in this study. The most frequently reported adverse events were mild, such as transient warmth (4%), burning (3%), nausea (3%), headache (3%), and pruritus (2%). Rapp et al. detailed a clinical trial that involved 274 patients from 37 centers known to have or suspected of having peripheral vascular disease at 1.5 T (11). Seven vessels were evaluated the infrarenal aorta, the left and right common iliac arteries, the left and right external iliac arteries, and the left and right common femoral arteries. A total of 251 patients with 1,646 vessels were evaluated for accuracy, and 140 patients with 237 diseased vessels were evaluated for sensitivity; 250 patients with 1,409 normal vessels were evaluated for specificity. An overall diagnostic accuracy of 84% to 90% was achieved compared to XRA. The increases for sensitivity, specificity, and accuracy were 14.5, 12.6, and 12.8%, respectively, compared to conventional MR angiography. Similar results were reported for a phase III clinical trial in 17 centers that included 178 patients known to have or suspected of having peripheral vascular disease (10) and for a phase III clinical trial in 18 centers that included 145 patients know to have or suspected of having renal artery disease (12).

### NIH Support

R01 CA82923, R24 CA83060, P20 CA91842, R01 HL38698.

## References

1 Henness S., Keating G.M. (2006). Gadofosveset. Drugs.
2 Shamsi K., Yucel E.K., Chamberlin P. (2006). A Summary of safety of gadofosveset (MS-325) at 0.03 mmol/kg body weight dose: Phase II and Phase III clinical trials data. Invest Radiol.
3 Kroft L.J., de Roos A. (1999). Blood pool contrast agents for cardiovascular MR imaging. J Magn Reson Imaging.
4 Lauffer R.B., Parmelee D.J., Ouellet H.S., Dolan R.P., Sajiki H., Scott D.M., Bernard P.J., Buchanan E.M., Ong K.Y., Tyeklar Z., Midelfort K.S., McMurry T.J., Walovitch R.C. (1996). MS-325: a small-molecule vascular imaging agent for magnetic resonance imaging. Acad Radiol.
5 Peyrin E., Guillaume Y.C., Guinchard C. (1999). Characterization of solute binding at human serum albumin site II and its geometry using a biochromatographic approach. Biophys J.
6 Lauffer R.B., Parmelee D.J., Dunham S.U., Ouellet H.S., Dolan R.P., Witte S., McMurry T.J., Walovitch R.C. (1998). MS-325: albumin-targeted contrast agent for MR angiography. Radiology.
7 Farooki A., Narra V., Brown J. (2004). Gadofosveset (EPIX/Schering). Curr Opin Investig Drugs.
8 Caravan P., Comuzzi C., Crooks W., McMurry T.J., Choppin G.R., Woulfe S.R. (2001). Thermodynamic stability and kinetic inertness of MS-325, a new blood pool agent for magnetic resonance imaging. Inorg Chem.
9 Eldredge H.B., Spiller M., Chasse J.M., Greenwood M.T., Caravan P. (2006). Species dependence on plasma protein binding and relaxivity of the gadolinium-based MRI contrast agent MS-325. Invest Radiol.
10 Goyen M., Edelman M., Perreault P., O'Riordan E., Bertoni H., Taylor J., Siragusa D., Sharafuddin M., Mohler E.R., Breger R., Yucel E.K., Shamsi K., Weisskoff R.M. (2005). MR angiography of aortoiliac occlusive disease: a phase III study of the safety and effectiveness of the blood-pool contrast agent MS-325. Radiology.
11 Rapp J.H., Wolff S.D., Quinn S.F., Soto J.A., Meranze S.G., Muluk S., Blebea J., Johnson S.P., Rofsky N.M., Duerinckx A., Foster G.S., Kent K.C., Moneta G., Middlebrook M.R., Narra V.R., Toombs B.D., Pollak J., Yucel E.K., Shamsi K., Weisskoff R.M. (2005). Aortoiliac occlusive disease in patients with known or suspected peripheral vascular disease: safety and efficacy of gadofosveset-enhanced MR angiography--multicenter comparative phase III study. Radiology.
12 McGregor, R., J. Vymazal, M. Martinez-Lopez, J. Neuwirth, P. Salgado, J.P. Beregi, A. Peduto, E. de la Pena-Almaguer, G.J. Slater, K. Shamsi, and E.C. Parsons, Jr., A multi-center, comparative, phase 3 study to determine the efficacy of gadofosveset-enhanced magnetic resonance angiography for evaluation of renal artery disease. Eur J Radiol, 2007
13 Aime S., Chiaussa M., Digilio G., Gianolio E., Terreno E. (1999). Contrast agents for magnetic resonance angiographic applications: 1H and 17O NMR relaxometric investigations on two gadolinium(III) DTPA-like chelates endowed with high binding affinity to human serum albumin. J Biol Inorg Chem.
14 Zhou X., Westlund P.O. (2005). 1H NMRD profiles and ESR lineshapes of Gd(III) complexes: a comparison between the generalized SBM and the stochastic Liouville approach. J Magn Reson.
15 Zech S.G., Eldredge H.B., Lowe M.P., Caravan P. (2007). Protein binding to lanthanide(III) complexes can reduce the water exchange rate at the lanthanide. Inorg Chem.
16 Mahfouz A.E. (2000). Ms-325 Epix. Curr Opin Investig Drugs.
17 Steger-Hartmann T., Graham P.B., Muller S., Schweinfurth H. (2006). Preclinical safety assessment of Vasovist (Gadofosveset trisodium), a new magnetic resonance imaging contrast agent for angiography. Invest Radiol.
18 Parmelee D.J., Walovitch R.C., Ouellet H.S., Lauffer R.B. (1997). Preclinical evaluation of the pharmacokinetics, biodistribution, and elimination of MS-325, a blood pool agent for magnetic resonance imaging. Invest Radiol.
19 Turetschek K., Floyd E., Helbich T., Roberts T.P., Shames D.M., Wendland M.F., Carter W.O., Brasch R.C. (2001). MRI assessment of microvascular characteristics in experimental breast tumors using a new blood pool contrast agent (MS-325) with correlations to histopathology. J Magn Reson Imaging.
20 Herborn C.U., Waldschuetz R., Lauenstein T.C., Goyen M., Lauffer R.B., Moeroey T., Debatin J.F., Ruehm S.G. (2002). Contrast-enhanced magnetic resonance imaging (MS-325) in a murine model of systemic lupus erythematosus. Invest Radiol.
21 Lin W., Abendschein D.R., Celik A., Dolan R.P., Lauffer R.B., Walovitch R.C., Haacke E.M. (1997). Intravascular contrast agent improves magnetic resonance angiography of carotid arteries in minipigs. J Magn Reson Imaging.
22 Prasad P.V., Cannillo J., Chavez D.R., Pinchasin E.S., Dolan R.P., Walovitch R., Edelman R.R. (1999). First-pass renal perfusion imaging using MS-325, an albumin-targeted MRI contrast agent. Invest Radiol.
23 Herborn C.U., Lauenstein T.C., Vogt F.M., Lauffer R.B., Debatin J.F., Ruehm S.G. (2002). Interstitial MR lymphography with MS-325: characterization of normal and tumor-invaded lymph nodes in a rabbit model. AJR Am J Roentgenol.
24 Grist T.M., Korosec F.R., Peters D.C., Witte S., Walovitch R.C., Dolan R.P., Bridson W.E., Yucel E.K., Mistretta C.A. (1998). Steady-state and dynamic MR angiography with MS-325: initial experience in humans. Radiology.
25 Perreault P., Edelman M.A., Baum R.A., Yucel E.K., Weisskoff R.M., Shamsi K., Mohler E.R. (2003). MR angiography with gadofosveset trisodium for peripheral vascular disease: phase II trial. Radiology.
26 Bluemke D.A., Stillman A.E., Bis K.G., Grist T.M., Baum R.A., D'Agostino R., Malden E.S., Pierro J.A., Yucel E.K. (2001). Carotid MR angiography: phase II study of safety and efficacy for MS-325. Radiology.
27 Goyen M., Shamsi K., Schoenberg S.O. (2006). Vasovist-enhanced MR angiography. Eur Radiol.